# N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-sulfhydryl-cyclic-arginine-glycine-aspartic acid dimeric peptide

Chemical name: | N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-sulfhydryl-cyclic-arginine-glycine-aspartic acid dimeric peptide
Abbreviated name: | [^18^F]FBEM-SRGD2
Synonym: | ^18^F-RGD2, [^18^F]FBEM-E[c(RGDyK)]_2_
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal /contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide)&WebEnv=0BLLjNep_4Na8W4oAlg1o8IYrXYJs6c8bHcZcM1npsIX2eqMoFrtJDI8lZfqNqMd47xB9b-jfArvt%40D4664A2364C62360_0155SID&WebEnvRq=1)]

N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-sulfhydryl-cyclic-arginine-glycine-aspartic acid dimeric peptide ([^18^F]FBEM-SRGD2) is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) of tumor vasculature and angiogenesis (1). ^18^F is a positron emitter with a physical half-life (t_½_) of 110 min.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature.

Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7). Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). Radiofluorination can generally be achieved through the functional groups of amino, carboxylic acid and sulfhydryl. ^18^F labeling of RGD peptide in most fluorinated peptide studies used ^18^F-synthons such as N-succinimidyl 4-[^18^F]fluorobenzoate to form a stable amide bond by reacting with primary amino groups of RGD peptides at the N terminus or the lysine side chain (1). One of the main concerns with this approach is the potential interference with the biological activities of these peptides. Cai et al. (1) suggested that ^18^F labeling of RGD peptides via the carboxylic acid group at the C terminus or internal glutamic/aspartic acid side chain might minimize the potential interference. They reported the successful use of a thiol-reactive ^18^F-synthron, ^18^F-FBEM, as the prosthetic group for labeling a sulfhydryl functionalized c(RGDyK) peptide (SRGD) via efficient alkylation of the free thiol group through the maleimido function (1). In the same study, the dimeric SRGD peptide (SRGD2) was similarly labeled as [^18^F]FBEM-SRGD2 and studied.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+synthesis&WebEnv=0I2bF98RYiQ70qDnPf_X9WlKizvFUUDnAUh7lSB_Vxc4SgCntBxAI7WmGjhsZce-S9o1O_eYPQl6Z%40D4664A2364C62360_0155SID&WebEnvR)]

The c(RGDyK) peptide was first prepared via solution cyclization of the fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by deprotection with trifluoroacetic acid (TFA) in the presence of the free radical scavenger triisopropylsilane (1, 9). The E[c(RGDyK)]_2_ peptide was prepared by coupling Boc-Glu-OH with two equivalents of monomeric RGD peptide followed by trifluoroacetic acid (TFA) cleavage (10). The E[c(RGDyK)]_2_ was conjugated to N-succinimidyl S-acetylthioacetate (SATA) by mixing E[c(RGDyK)]_2_ in sodium borate (Na_2_B_4_O_7_) buffer (pH 8.5) with SATA in dimethyl sulfoxide (1). The yield was 65%. The crude SATA-E[c(RGDyK)]_2_ was then dissolved in water and mixed with L hydroxylamine at pH 6.0 for 2 h to yield the SRGD2. The final product was purified by semipreparative high-performance liquid chromatography (HPLC). The overall yield was 50%. The identity of the SRGD2 peptide (C_29_H_43_N_9_O_9_S) was confirmed by the matrix-assisted laser desorption/ionization time-of-flight mass spectroscopy. FBEM was obtained by reacting N-(2-aminoethyl)maleimide with N-succinimidyl 4-fluorobenzoate in Na_2_B_4_O_7_ (pH 8.5) at 50ºC for 20 min. The reaction was quenched by 2% trifuoroacetic acid. The yield was 85% after HPLC purification.

Cai et al. (1) reported the radiolabeling of [^18^F]FBEM-SRGD2 by using ^18^F-FBEM, which was first prepared from N-succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) (11, 12). [^18^F]SFB in acetonitrile was then mixed with N-(2-aminoethyl)maleimide and N,N-diisopropylethylamine. The reaction mixture was heated at 40ºC for 20 min and then quenched by trifluoroacetic acid. [^18^F]FBEM purified by HPLC was obtained with a total reaction time of 150 ± 20 min. The nondecay-corrected radiochemical yield was 5 ± 2% (on the basis of 18F-F−) with a specific activity of 150-200 TBq/mmol (4,050-5,400 Ci/mmol). Purified [^18^F]FBEM in phosphate buffered saline was mixed the SRGD2 peptide in dimethyl sulfoxide and tris(2-carboxyethyl)phosphine hydrochloride in water. The pH of the mixture was adjusted to 7.0-7.5 and incubated at room temperature for 20 min. The resulting [^18^F]FBEM-SRGD2 was purified by HPLC. The radiochemical yield was 85 ± 5% (nondecay-corrected) on the basis of 18F-FBEM, The total reaction time including final HPLC purification was ~200 ± 25 min. The overall decay-corrected radiochemical yield was 20 ± 4% (n = 5), and the specific activity was 100-150 TBq/mmol (2,700-4,050 Ci/mmol). The radiochemical purity was >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+in+vitro&WebEnv=0a5II5Gs_JOpUmsnQikbvuPGARlXBgKwCgwH9GaXPnG-a7NAOoYeqYwolMM4vvyMkqFnISiJ3cZsp%40D4664A2364C62360_0155SID&WebEnvRq=)]

Cai et al. (1) determined the octanol/water partition coefficient (Log P) of [^18^F]FBEM-SRGD2 to be −1.69 ± 0.02, which indicated that this radioligand was hydrophilic. In comparison, the Log P of [^18^F]FBEM-SRGD was 0.93 ± 0.02. In vitro cell-binding affinity studies of the unlabeled FBEM-SRGD2 was conducted in U87MG glioblastoma cells with ^125^I-echistatin as the integrin α_v_β_3_ specific radioligand. The inhibition constant (IC_50_) for FBEM-SRGD2 was determined to be 55.1 ± 6.5 nM. In comparison, the IC_50_ for E[c(RGDyK)]_2_ was determined to be 26.1 ± 3.2 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+rodentia&WebEnv=0f8W2adxgufdPEvIqGnB3mHoFAaNf1vIR3nXXc8cwSwi7exEDpOXWAccr9Zfy1_6f9cwG471xstYC%40D4664A2364C62360_0155SID&WebEnvRq)]

Biodistribution studies of [^18^F]FBEM-SRGD2 were conducted in nude mice bearing the U87MG glioblastoma on the right front leg and the MDA-MB-435 breast cancer carcinoma on the left mammary fat pad (1). Both tumor volumes reached ~30-400 mm^3^. Each mouse received one MBq (27 μCi) of [^18^F]FBEM-SRGD2 by i.v. administration. At 60 min, the radioactivity levels (n = 3) in percent dose per g (% ID/g) detected in the U87MG tumor and MDA-MB-435 tumor were 2.71 ± 0.19 and 5.25 ± 0.26, respectively. When blocked by coinjection of 10 mg/kg c(RGDyK), the U87MG tumor level decreased >5-fold to 0.52 ± 0.26% ID/g (P<0.01). Similar decrease to ~0.8% ID/g (Figure 3) was also seen in the MDA-MB-435 tumor. The authors suggested that the steady increase of MDA-MB-435 tumor activity over time might indicate internalization of the radiolabeled peptide. [^18^F]FBEM-SRGD2 was relatively hydrophilic and was primarily excreted by the kidney. The kidney radioactivity level at 10 min was 11.40 ± 0.22% ID/g. Extrapolation from Figure 3 of the article estimated that the radioactivity level of the kidney decreased rapidly to ~5% ID/g at 60 min. The radioactivity levels of other major organs were ~4.5% ID/g, ~3% ID/g, and ~3% ID/g for the blood, liver, and intestine at 10 min, respectively. At 60 min, these levels appeared to change to ~1% ID/g, ~2% ID/g, and ~2% ID/g, respectively. The metabolic stability of [^18^F]FBEM-SRGD2 was also studied in mouse blood and urine samples, and tissues homogenates of the liver, kidneys, and U87MG tumor at 60 min after administration. HPLC analysis showed that the percentages (%) of unchanged [^18^F]FBEM-SRGD2 were 80.7 (blood), 41.7(urine), 59.7 (liver), 77.5 (U87MG tumor), and 85.8 (kidney). The metabolites were not identified, but they were all more polar than the intact compound.

MicroPET imaging of 3.7 MBq (100 μCi) [^18^F]FBEM-SRGD2 was performed in nude mice bearing both the s.c. U87MG tumor and orthotopic MDA-MB-435 tumor (1). The radioligand appeared to be excreted predominantly through the kidneys. Most radioactivity in nontargeted tissues were cleared at 60 min. With coinjection of 10 mg/kg unlabeled c(RGDyK), the radioactivity level in the U87MG tumor decreased from 2.21% ID/g to 0.94% ID/g at 30 min and from 1.73% ID/g to 0.44% ID/g at 60 min. No bone radioactivity was visualized in all of the imaging studies, and the authors suggested that this might indicate no significant amount of ^18^F label was released from the radioligand.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+(dog+OR+rabbit+OR+pig+OR+sheep)&WebEnv=0lm4alv-2HCxC8e5RE3UcBkg5Er7OQct12zsixw-5BK4hv0paJj02SWyPp4qgQ9c2PBfpXFHkISyI%40D4664A2364)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+(primate+NOT+human)&WebEnv=0kkMh4y2inxOXWNkWiV0bqO0sAdEBRADMKKYVnn_Sr4yl6iKDVNKy2An4DI64c9iCSt2TXQ90s-TY%40D4664A2364C62360_0155S)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+human&WebEnv=0SffZNl7ihnQdRkfTQUS6M8Z4Nt545Ampfi4CXNXd3PL91KiaYZbG7pigmprTtZS6oBjCa9wGABOC%40D4664A2364C62360_0155SID&WebEnvRq=1)]

No publication is currently available.

## NIH Support

NIH CA93862, NCI P50 CA114747.

## References

1 Cai W., Zhang X., Wu Y., Chen X. (2006). A thiol-reactive 18F-labeling agent, N-[2-(4-18F-fluorobenzamido)ethyl]maleimide, and synthesis of RGD peptide-based tracer for PET imaging of alpha v beta 3 integrin expression. J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
10 Chen X., Sievers E., Hou Y., Park R., Tohme M., Bart R., Bremner R., Bading J.R., Conti P.S. (2005). Integrin alpha v beta 3-targeted imaging of lung cancer. Neoplasia.
11 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
12 Chen X., Park R., Hou Y., Khankaldyyan V., Gonzales-Gomez I., Tohme M., Bading J.R., Laug W.E., Conti P.S. (2004). MicroPET imaging of brain tumor angiogenesis with 18F-labeled PEGylated RGD peptide. Eur J Nucl Med Mol Imaging.